# ^99m^Tc≡Nitrido(diphosphine)-Cys-β-Ala-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_

Chemical name: | ^99m^Tc≡Nitrido(diphosphine)-Cys-β-Ala-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_
Abbreviated name: | ^99m^TcN(PNP6)-Cys-BBN, ^99m^TcN(PNP6)-Cys-β-Ala-BBN(7-14)NH_2_
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | SPECT, gamma planar imaging
Source of signal\contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PNP6+BBN)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on CNS and GI tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely neuromedin B (NMB or BB1), the GRPR subtype (BB2), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Faintuch et al. (7) used ^99m^Tc-nitrido(diphosphine) for labeling Cys-β-Ala-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (Cys-BBN). ^99m^Tc≡Nitrido(diphosphine)-Cys-BBN (^99m^TcN(PNP6)-Cys-BBN) is being evaluated as a single-photon emission computed tomography (SPECT) imaging agent of GRPR in nude mice bearing PC-3 human prostate cancer cells.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PNP6+BBN+synthesis)]

The ^99m^Tc-nitrido precursor species were prepared by the addition of succinic acid dihydrazide, nitrido-donor ligand, and stannous chloride to 0.5 ml aqueous Na^99m^TcO_4_ (7). The solution was incubated for 30 min at room temperature. After incubation, 0.045 mmol Cys-BBN and 3 µg diphosphine were added to the solution, which was then heated for 60 min at 100°C. ^99m^TcN(PNP6)-Cys-BBN was purified with Sep-Pak with a radiochemical purity of >96% and a radiochemical yield of >97%. The specific activity of the purified product was not reported. The measured log P value was 0.98. ^99m^TcN(PNP6)-Cys-BBN was >93% intact after 4 h in saline and in the presence of 100 mM cysteine.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PNP6+BBN+in+vitro)]

Faintuch et al. (7) performed in vitro internalization of ^99m^TcN(PNP6)-Cys-BBN in cultured PC-3 cancer cells. PC-3 cells exhibited a rapid internalization with 8.9% of radioactivity accumulated at 30 min and 15.5% accumulated at 120 min after incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PNP6+BBN+rodentia)]

Faintuch et al. (7) performed biodistribution studies of ^99m^TcN(PNP6)-Cys-BBN in nude mice bearing PC-3 xenografts. Tumor accumulation was 1.2 ± 0.3% injected dose (ID)/g at 90 min. The organs with the highest uptake (~7% ID/g) were the liver, small intestine, and pancreas; little radioactivity (~0.4% ID/g) accumulated in the muscle, blood, and bone. Tumor/blood and tumor/muscle ratios were 3.1 and 2.7, respectively. Co-administration of excess Cys-BBN inhibited tumor accumulation by 33%, whereas the accumulation in the pancreas was inhibited by 80% with little effect in the other tissues. SPECT imaging in nude mice bearing PC-3 xenografts was performed with 18.5–37 MBq (0.5–1.0 mCi) of ^99m^TcN(PNP6)-Cys-BBN. The tumors were clearly visualized with 1.7% ID at 90 min after injection. Co-administration of excess Cys-BBN substantially inhibited the radioactivity in the tumors (59%).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PNP6+BBN+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PNP6+BBN+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PNP6+BBN+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Faintuch B.L., Teodoro R., Duatti A., Muramoto E., Faintuch S., Smith C.J. (2008). Radiolabeled bombesin analogs for prostate cancer diagnosis: preclinical studies. Nucl Med Biol.